# ^99m^Tc-S-acetylmercaptoacetyltriserine-stromal-derived factor 1α

Chemical name: | ^99m^Tc-S-acetylmercaptoacetyltriserine- stromal-derived factor 1α
Abbreviated name: | ^99m^Tc-MAS_3_-SDF-1α
Synonym: | CXCL12
Agent Category: | Chemokine
Target: | CXCR4
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here to view protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=156416009) and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=156416008) sequence of SDFα1

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SDF+1+alpha)]

The immune system is largely modulated by a variety of small, glycosylated proteins called chemokines, which vary in size from ~5 to 15 kDa. These molecules possess strong chemotactic or leukocyte activation properties and are structurally related. They are classified by the International Union of Immunological Societies and the World Health Organization into four groups designated as C, CC, CXC, and CX_3_C on the basis of the location of the cysteine residues in the mature protein (1). The chemokines interact with several different 7-transmembrane G-protein–coupled receptors that are designated according to the chemokine subfamily name followed by the letter “R” (for receptor) and a number based on the chronological order of its identification within a subfamily (for details see Thorpe (1)). The stromal-derived factor-1α (SDF-1α or CXC12) is a member of the CXC family of chemokines that binds to the CXCR4. SDF-1α has an important role in several immunological processes, including hematopoiesis, vasculogenesis, neuronal development, and immune cell mobilization (2-4). Because of their role in several diverse physiological processes, SDF-1α and its receptor (CXCR4) have been implicated in a variety of pathological conditions such as inflammation, cancer, and HIV infections (5-7). The United States Food and Drug Administration has approved several clinical trials (http://clinicaltrials.gov/ct2/results?term=SDF) to evaluate the use of SDF-1α and CXCR4 receptors in cancer and myocardial infarction (MI) treatment.

SDF-1α and its receptor have also been shown to be involved in the neointimal recruitment of smooth muscle cell (SMC) progenitors, probably as a response to SMC apoptosis, during restenosis and cardiac allograft vasculopathy (8). In addition, SDF-1α and CXCR4 are expressed on hematopoietic stem cells and endothelial progenitor cells, are necessary for cardiogenesis, and have a role in cardiac myocyte contraction in rats (9-11). The levels of the chemokine and its receptor are elevated during cardiac dysfunction and in the hearts of patients experiencing congestive heart failure (12-14). Chemokines have also been shown to mobilize stem cells after MI, probably to repair the injured myocardium by the re-expression of SDF-1α in the tissue, which could possibly help direct the homing of stem cells to the injured area (15, 16). The exact mechanism(s) of how chemokines and their receptors bring about these effects in the injured cardiac tissue are not clear. In this regard it becomes important to investigate the chemokines and their receptors noninvasively in an in vivo setting to understand the role and functioning of these molecules in the myocardium. Misra et al. labeled SDF-1α with radioactive technetium (^99m^Tc) and used it to quantify CXCR4 expression in a rat MI model (17). The biodistribution of ^99m^Tc-labeled SDF-1α was also studied in animals.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+SDF+synthesis)]

^99m^Tc-SDF-1α was synthesized using an N-hydroxysuccinimide (NHS) ester of ^99m^Tc-S-acetylmercaptoacetyltriserine (^99m^Tc-MAS_3_) as described by Misra et al. (17). ^99m^Tc-MAS_3_-NHS (purity >99%) was prepared in dimethylsulfoxide (DMSO) as described elsewhere (18). Recombinant murine SDF-1α was obtained as a dry powder from commercial sources and resuspended in DMSO. The SDF-1α suspension was mixed with ^99m^Tc-MAS_3_-NHS after the addition of 4 M triethylamine and stirred at room temperature for 1 h. Labeled SDF-1α was purified with gel filtration on a 60-Å Diol gel filtration column (GFC) on phosphate-buffered saline (PBS) (pH 7.4). The GFC-purified ^99m^Tc-MAS_3_-SDF-1α was reported to have a specific activity of 8.0 × 10^7^ MBq/mmol (2,166 Ci/mmol). Stability of the labeled product was studied with GFC chromatography after boiling it in PBS for 5 min, with or without dithiothreitol, and by incubating it in 100% calf serum for 4 h at 37°C (17). No dissociation or transmetallation was reported under these conditions, and >98% of ^99m^Tc-MAS_3_-SDF-1α was intact as determined with GFC chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+SDF+in+vitro)]

The affinity and specificity of ^99m^Tc-MAS_3_-SDF-1α for CXCR4 in PC-3 human prostate cancer cells transduced with an adenoviral vector coexpressing CXCR4 and green fluorescence protein (this was used as an indicator to confirm that the cells were transduced with the vector) was determined using a live-cell homologous competition assay as described by Misra et al. (18). Control cells were either transduced with an adenoviral vector coexpressing bone morphogenic protein-2 and green fluorescence protein or untransduced cells. A high specificity for CXCR4 was exhibited by ^99m^Tc-MAS_3_-SDF-1α with an affinity of 1.0±0.1 nM, and the maximal binding was 2.6 × 10^5^ binding sites per cell. No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+SDF+rodentia)]

The biodistribution and clearance of ^99m^Tc-MAS_3_-SDF-1α was investigated in Sprague-Dawley inbred rats (the number of animals used was not reported) with or without MI as described by Misra et al. (17). The animals were administered intravenously with the radioactive compound through the retroorbital sinus, and blood was collected from the tail vein at various times from 0 to 120 min after administration. The main organs (stomach, lungs, liver, etc.) of the animals were obtained 2 h after administration of the radiochemical, washed twice with PBS, weighed, and counted for radioactivity. Heart tissue from the MI animals was divided into infarcted and noninfarcted tissue for quantitation. Control animals were also injected with ^99m^Tc-MAS_3_ alone. The blood half-life of ^99m^Tc-MAS_3_-SDF-1α was determined to be 25.8 ± 4.6 min compared to 5.0 ± 1.0 min for ^99m^Tc-MAS_3_ alone (17). An uptake of <0.1% of the injected dose/gram tissue (% ID/g) was noted in the major organs, except the kidneys, with no uptake in the brain. The kidneys had ~0.5% ID/g, and the radioactivity was detected primarily in the urine (the exact % ID/g was not reported) with a total of 73.8 ± 6.1% ID/g in the excrement, including feces.

Using rats with an induced MI that were injected with ^99m^Tc-MAS_3_-SDF-1α, the expression of CXC4 was determined to be increased in the MI tissue (17). The MI tissue showed a five-fold increase (P < 0.0001) in ^99m^Tc-MAS_3_-SDF-1α binding (0.57 ± 0.04% ID/g) compared with the noninfarcted or normal heart tissue (0.11 ± 0.1% ID/g). Blocking studies, using unlabelled ligand, were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+SDF+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+SDF+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

This work was supported by NIH grants R01-CA-115296, R01-HL-073458 and R01-HL-078691.

## References

1 Thorpe R. (2003). Chemokine/chemokine receptor nomenclature IUIS/WHO subcommittittee on chemokine nomenclature. Cytokine.
2 Hildebrandt M., Schabath R. (2008). SDF-1 (CXCL12) in haematopoiesis and leukaemia: impact of DPP IV/CD26. Front Biosci.
3 Arya M., Ahmed H., Silhi N., Williamson M., Patel H.R. (2007). Clinical importance and therapeutic implications of the pivotal CXCL12-CXCR4 (chemokine ligand-receptor) interaction in cancer cell migration. Tumour Biol.
4 Barbieri F., Bajetto A., Porcile C., Pattarozzi A., Schettini G., Florio T. (2007). Role of stromal cell-derived factor 1 (SDF1/CXCL12) in regulating anterior pituitary function. J Mol Endocrinol.
5 MacDermott R.P. (1999). Chemokines in the inflammatory bowel diseases. J Clin Immunol.
6 Muller A., Homey B., Soto H., Ge N., Catron D., Buchanan M.E., McClanahan T., Murphy E., Yuan W., Wagner S.N., Barrera J.L., Mohar A., Verastegui E., Zlotnik A. (2001). Involvement of chemokine receptors in breast cancer metastasis. Nature.
7 Berger E.A. (1998). Introduction: HIV co-receptors solve old questions and raise many new ones. Semin Immunol.
8 Schober A., Zernecke A. (2007). Chemokines in vascular remodeling. Thromb Haemost.
9 Yamaguchi J., Kusano K.F., Masuo O., Kawamoto A., Silver M., Murasawa S., Bosch-Marce M., Masuda H., Losordo D.W., Isner J.M., Asahara T. (2003). Stromal cell-derived factor-1 effects on ex vivo expanded endothelial progenitor cell recruitment for ischemic neovascularization. Circulation.
10 Aukrust P., Ueland T., Muller F., Andreassen A.K., Nordoy I., Aas H., Kjekshus J., Simonsen S., Froland S.S., Gullestad L. (1998). Elevated circulating levels of C-C chemokines in patients with congestive heart failure. Circulation.
11 Pyo R.T., Sui J., Dhume A., Palomeque J., Blaxall B.C., Diaz G., Tunstead J., Logothetis D.E., Hajjar R.J., Schecter A.D. (2006). CXCR4 modulates contractility in adult cardiac myocytes. J Mol Cell Cardiol.
12 Behr T.M., Wang X., Aiyar N., Coatney R.W., Li X., Koster P., Angermann C.E., Ohlstein E., Feuerstein G.Z., Winaver J. (2000). Monocyte chemoattractant protein-1 is upregulated in rats with volume-overload congestive heart failure. Circulation.
13 Shioi T., Matsumori A., Kihara Y., Inoko M., Ono K., Iwanaga Y., Yamada T., Iwasaki A., Matsushima K., Sasayama S. (1997). Increased expression of interleukin-1 beta and monocyte chemotactic and activating factor/monocyte chemoattractant protein-1 in the hypertrophied and failing heart with pressure overload. Circ Res.
14 Aukrust P., Damas J.K., Gullestad L., Froland S.S. (2001). Chemokines in myocardial failure -- pathogenic importance and potential therapeutic targets. Clin Exp Immunol.
15 Abbott J.D., Huang Y., Liu D., Hickey R., Krause D.S., Giordano F.J. (2004). Stromal cell-derived factor-1alpha plays a critical role in stem cell recruitment to the heart after myocardial infarction but is not sufficient to induce homing in the absence of injury. Circulation.
16 Zhang M., Mal N., Kiedrowski M., Chacko M., Askari A.T., Popovic Z.B., Koc O.N., Penn M.S. (2007). SDF-1 expression by mesenchymal stem cells results in trophic support of cardiac myocytes after myocardial infarction. Faseb J.
17 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 Expression in Myocardial Infarction Using 99mTc-Labeled SDF-1{alpha}. J Nucl Med.
18 Misra P., Humblet V., Pannier N., Maison W., Frangioni J.V. (2007). Production of multimeric prostate-specific membrane antigen small-molecule radiotracers using a solid-phase 99mTc preloading strategy. J Nucl Med.